# Cy5.5-Cyclo(CGNSNPKSC)

Chemical name: | Cy5.5-Cyclo(CGNSNPKSC)
Abbreviated name: | Cy5.5-GX1
Synonym:
Agent category: | Peptide
Target: | Tumor vasculature
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1)]

Angiogenesis is an essential process in the development of new blood vessels in normal physiological states and in diseases (1, 2). Targeting of tumor vasculature is a promising strategy for tumor imaging and therapy because tumor growth and metastasis largely depend on angiogenesis (3, 4). A cyclic 9-mer peptide (CGNSNPKSC (GX1)) was initially identified as a recognition motif for binding to the human gastric tumor vasculature (5-7). GX1 has also been shown to bind to a variety of human cancer vasculatures. The molecular target of GX1 has not been identified; however, GX1 inhibits endothelial cell proliferation in vitro and neovascularization in vivo. The Lys (K) residue of GX1 was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in mice bearing U89MG human glioblastoma tumors (8). Cy5.5-GX1 exhibited high near-infrared (NIR) fluorescence intensity in U89MG tumors in nude mice.

### Related Resource Links:

- Chapters in MICAD (GX1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GX1+AND+micad%5Bbook%5D))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+synthesis)]

The Boc-protected GX1 peptide was obtained using solid-phase synthesis (8). Cy5.5-N-hydroxysuccinimide (NHS) ester (500 nmol) was used to conjugate the peptide (500 nmol) for 2 h at 45°C. The NHS ester of Cy5.5 reacted with the Ɛ-amino group of the Lys residue of the peptide. The Boc-protected Cy5.5-GX1 was isolated with high-performance liquid chromatography (HPLC), with 66% yield. Trifluoracetic acid was used to remove the Boc-protecting group to form Cy5.5-GX1, with 76% yield and >97% chemical purity after HPLC purification. Mass spectroscopy analysis confirmed a 1:1 addition of Cy5.5 to GX1. Fluorescence excitation and emission maxima of Cy5.5 were 675 nm and 695 nm, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+and+in+vitro)]

Flow cytometry analysis showed that 6%, 12%, and 25% of U89MG cells were positive after incubation with 0.5, 1, and 4 nmol Cy5.5-GX1 for 60 min at 4°C (8). Confocal microscopy showed internalization of fluorescence activity inside the cells. Neither binding affinity of the derivatized peptide for the tumor vasculature nor blocking studies were performed with unlabeled GX1.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+rodentia)]

Chen et al. (8) performed NIR fluorescence imaging of nude mice (n = 3) bearing U89MG tumors at 0.5–24 h after intravenous injection of 1 nmol Cy5.5-GX1. The tumor accumulation of Cy5.5-GX1 could be clearly visualized from 1 h to 24 h, with a maximum contrast at 4–8 h. The tumor/background ratio was ~4 at 8 h after injection. Co-injection of GX1 (20 µmol/kg) inhibited the fluorescence signal to near background level at 4 h after injection (P < 0.05). Ex vivo NIR fluorescence imaging of tissues at 24 h after injection showed that the tissues with the highest signals (photons/s/cm^2^/steradian) were the tumor (1.77 x 10^8^) and liver (0.44 x 10^8^), followed by the kidney (0.22 x 10^8^), lung (<0.2 x 10^8^), spleen (<0.2 x 10^8^), heart (<0.2 x 10^8^), blood (<0.2 x 10^8^), and muscle (<0.2 x 10^8^). The tumor/muscle, tumor/liver, and tumor/kidney ratios were 15.21 ± 0.84, 4.02 ± 0.13, and 7.98 ± 0.44, respectively, whereas the corresponding values for the blocked group were 6.95 ± 0.75, 2.79 ± 0.35, and 4.67 ± 0.55, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+human)]

No publication is currently available.

## References

1 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
2 Folkman J. (2007). Angiogenesis: an organizing principle for drug discovery?. Nat Rev Drug Discov.
3 Abdollahi A., Folkman J. (2010). Evading tumor evasion: current concepts and perspectives of anti-angiogenic cancer therapy. Drug Resist Updat.
4 Thorpe P.E. (2004). Vascular targeting agents as cancer therapeutics. Clin Cancer Res.
5 Chen B., Cao S., Zhang Y., Wang X., Liu J., Hui X., Wan Y., Du W., Wang L., Wu K., Fan D. (2009). A novel peptide (GX1) homing to gastric cancer vasculature inhibits angiogenesis and cooperates with TNF alpha in anti-tumor therapy. BMC Cell Biol.
6 Hui X., Han Y., Liang S., Liu Z., Liu J., Hong L., Zhao L., He L., Cao S., Chen B., Yan K., Jin B., Chai N., Wang J., Wu K., Fan D. (2008). Specific targeting of the vasculature of gastric cancer by a new tumor-homing peptide CGNSNPKSC. J Control Release.
7 Zhi M., Wu K.C., Dong L., Hao Z.M., Deng T.Z., Hong L., Liang S.H., Zhao P.T., Qiao T.D., Wang Y., Xu X., Fan D.M. (2004). Characterization of a specific phage-displayed Peptide binding to vasculature of human gastric cancer. Cancer Biol Ther.
8 Chen, K., L.P. Yap, R. Park, X. Hui, K. Wu, D. Fan, X. Chen, and P.S. Conti, A Cy5.5-labeled phage-displayed peptide probe for near-infrared fluorescence imaging of tumor vasculature in living mice. Amino Acids, 2011